# ^89^Zr-N-Succinyldesferrioxamine-DN30

Chemical name: | ^89^Zr-N-Succinyldesferrioxamine-DN30
Abbreviated name: | ^89^Zr-DN30
Synonym:
Agent category: | Antibody
Target: | MET, also known as the tyrosine kinase receptor for hepatocyte growth factor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^89^Zr
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zr%20DN30)]

MET is a proto-oncogene that encodes a protein MET, also known as c-Met or hepatocyte growth factor receptor (HGFR) (1). MET is a membrane receptor that is essential for embryonic development and wound healing. Hepatocyte growth factor (HGF) is the only known ligand of MET. MET is normally expressed by stem cells, progenitor cells and cells of epithelial origin, whereas expression of HGF is restricted to cells of mesenchymal origin. Upon HGF stimulation, MET induces several biological responses that lead invasive growth (2). Abnormal MET activation in cancer correlates with poor prognosis, where de-regulated MET triggers tumor growth, induces angiogenesis, and activates metastasis (3). MET is deregulated in many types of human malignancies, including cancers of kidney, liver, stomach, breast, and brain (2, 4, 5). Monoclonal antibody DN30 is directed against the extracellular domain of MET with a K_d_ of 2.64 nM (6). Inhibition of HGFR function with DN30 has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis. Perk et al. (7) prepared ^89^Zr-N-succinyldesferrioxamine-DN30 (^89^Zr-DN30) for imaging MET expression in tumors.

### Related Resource Links:

- Chapters in MICAD (c-Met (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=c-Met+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (c-Met (http://www.ncbi.nlm.nih.gov/gene/4233)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (c-Met (http://www.ncbi.nlm.nih.gov/omim/?term=c-Met))
- Clinical trials (c-Met (http://www.clinicaltrials.gov/ct2/results?term=c-Met))
- Drug information in FDA (c-Met (http://google2.fda.gov/search?q=c-Met&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=10&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zr%20DN30+synthesis)]

N-Succinyldesferrioxamine (N-sucDf) B-tetrafluorphenol-Fe and DN30 were incubated in sodium carbonate buffer (pH, 9.5) for 30 min at room temperature (7). To the mixture, an EDTA solution was added and the mixture was incubated for 30 min at 35ºC. N-sucDf-DN30 was isolated from the incubation mixture with a PD-10 column. There was ~1 chelate group per antibody. N-sucDf-DN30 was mixed with ^89^Zr-oxalate. The mixture was incubated for 45 min at room temperature. ^89^Zr-DN30 had a radiochemical purity of >95% and a specific activity 8.2-10.6 MBq/nmol (0.22-0.29 mCi/nmol) with a labeling yield of >70%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zr%20DN30+in+vitro)]

Radioimmunoreactivity of ^89^Zr-DN30 for MET was determined by measuring of ^89^Zr-DN30 binding to GTL-16 cells to be >95% at infinite antigen excess (7).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zr%20DN30+rodentia)]

Perk et al. (7) performed biodistribution studies of 0.28 MBq (0.008 mCi,) ^89^Zr-DN30 (0.66 nmol) in nude mice bearing human gastric carcinoma cell line GTL-16 (high MET expression) or the HNSCC cell line FaDu (low MET expression) xenografts. GTL-16 tumor uptake values were 12.2% ID/g (percentage injected dose per gram) at 1 d, 17.3% ID/g at 2 d, 18.1% ID/g at 3 d, and 19.6% ID/g at 5d. The radioactivity level in the blood was 17.1, 13.3, 10.6 and 8.8% ID/g at 1, 2, 3, and 5 d, respectively. The organs with the highest uptake were the liver (8.4% ID/g), spleen (7.9% ID/g), lung (4.5% ID/g), and kidneys (3.5% ID/g) with the lowest radioactivity in the muscle (1.2% ID/g) at 3 d after injection. The tumor/muscle ratio was 15. On the other hand, the FaDu tumor uptake was lower than GTL-16 tumor with only 7.8% ID/g and the tumor/muscle ratio of 7 at d 3. PET imaging revealed that GTL-16 tumors as small as 11 mg were readily visualized as early as 1 d and up to 4 d after injection. The liver and spleen were also visualized. FaDu tumors were less pronounced than the GTL-16 tumors. Immunohistochemistry with DN30 was performed on GTL-16 and FaDu xenografts showed that the expression of MET was higher in the GTL-16 tumor sections than that of FaDu tumor sections. No blocking experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zr%20DN30+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zr%20DN30+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zr%20DN30+human)]

No publication is currently available.

## References

1 Boccaccio C., Comoglio P.M. (2006). Invasive growth: a MET-driven genetic programme for cancer and stem cells. Nat Rev Cancer.
2 Di Renzo M.F., Olivero M., Giacomini A., Porte H., Chastre E., Mirossay L., Nordlinger B., Bretti S., Bottardi S., Giordano S., et al. (1995). Overexpression and amplification of the met/HGF receptor gene during the progression of colorectal cancer. Clin Cancer Res.
3 Lengyel E., Prechtel D., Resau J.H., Gauger K., Welk A., Lindemann K., Salanti G., Richter T., Knudsen B., Vande Woude G.F., Harbeck N. (2005). C-Met overexpression in node-positive breast cancer identifies patients with poor clinical outcome independent of Her2/neu. Int J Cancer.
4 Smith H.S., Stern R., Liu E., Benz C. (1991). Early and late events in the development of human breast cancer. Basic Life Sci.
5 Di Renzo M.F., Olivero M., Serini G., Orlandi F., Pilotti S., Belfiore A., Costantino A., Vigneri R., Angeli A., Pierotti M.A., et al. (1995). Overexpression of the c-MET/HGF receptor in human thyroid carcinomas derived from the follicular epithelium. J Endocrinol Invest.
6 Petrelli A., Circosta P., Granziero L., Mazzone M., Pisacane A., Fenoglio S., Comoglio P.M., Giordano S. (2006). Ab-induced ectodomain shedding mediates hepatocyte growth factor receptor down-regulation and hampers biological activity. Proc Natl Acad Sci U S A.
7 Perk L.R., Stigter-van Walsum M., Visser G.W., Kloet R.W., Vosjan M.J., Leemans C.R., Giaccone G., Albano R., Comoglio P.M., van Dongen G.A. (2008). Quantitative PET imaging of Met-expressing human cancer xenografts with (89)Zr-labelled monoclonal antibody DN30. Eur J Nucl Med Mol Imaging.